# ^99m^Tc-2-[Bis-(2-mercaptoethyl)]aminoethanethiol-4-isocyano-N-[2-(2-methyl-5-nitro-1H-imidazol-1-yl)ethyl]butanamide

Chemical name: | ^99m^Tc-2-[Bis-(2-mercaptoethyl)]aminoethanethiol-4-isocyano-N-[2-(2-methyl-5-nitro-1H-imidazol-1-yl)ethyl]butanamide | [image]
Abbreviated name: | ^99m^Tc-NS_3_M1 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Hypoxia | [image]
Target Category: | Others | [image]
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of the ligands M1 and M2

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=hypoxia%20and%20imaging%20and%20review)]

^99m^Tc-2-[Bis-(2-mercaptoethyl)]aminoethanethiol (NS_3_)-4-isocyano-N-[2-(2-methyl-5-nitro-1H-imidazol-1-yl)ethyl]butanamide (M1), abbreviated as ^99m^Tc-NS_3_M1, is a ^99m^Tc-'4+1'-labeled 5-nitroimidazole derivative synthesized by Giglio et al. for single-photon emission computed tomography (SPECT) of hypoxia (1).

Solid tumors are characterized by hypoxia because of the rapid growth of tumors and the structural abnormality of tumor vasculature (2, 3). Hypoxia caused by perfusion-limited O_2_ delivery is usually transient and is therefore also called “acute hypoxia.” Correspondingly, hypoxia caused by the increased diffusion distance is called "diffusion-limited hypoxia" or "chronic hypoxia" (3). The key molecular event of hypoxia is the upregulation of hypoxia-inducible factor, which leads to increased expression of various hypoxia-responsive elements (4). Tumors that experience hypoxia exhibit enhanced angiogenesis, increased anaerobic metabolism, rapid growth, and resistance to chemoradiotherapy (3, 5).

The diverse techniques that have been used to assess hypoxia can be divided into direct and indirect measurements, with the polarographic needle electrode as the gold standard measurement (6, 7). Because of the obvious limitations of direct measurements, noninvasive imaging with exogenous probes has been intensively investigated, which focuses on the mapping of hypoxia throughout tumors and the prediction of tumor prognosis. To date, most chemical probes developed for positron emission tomography (PET) and SPECT are metronidazole derivatives (3, 6-8). These compounds undergo reductive metabolism and form stable adducts with intracellular macromolecules under hypoxic conditions (oxygen pressure <10 mmHg). In normoxic tissues, these compounds are rapidly reoxidized and wash out quickly from the cells.

Giglio et al. synthesized ^99m^Tc-NS_3_M1 and ^99m^Tc-NS_3_M2 by labeling two 5-nitroimidazole derivatives, M1 and 1-(4-isocyanobutanoyl)-4-[2-(2-methyl-5-nitro-1H-imidazol-1-yl)ethyl]piperazine (M2) through preparation of their corresponding ^99m^Tc-(4+1) complexes (1). Metronidazole can be attached with chelating groups that enable the coordination of ^99m^Tc without losing its specific recognition to target sites in vivo. The investigators selected the ^99m^Tc-(4+1) core for labeling because this approach yields high specific activity tracers while preserving the biological activity of the ligands (1). The ^99m^Tc-(4+1) complexes developed by Giglio et al. are oxo-free with the metal at oxidation state +3, formed by combination of the tripodal chelator 2,2',2''-nitrilotris(ethanethiol) and a monodentate isocyanide (1). The non-polar isocyanide building block is stable against ligand exchange in vivo and provides ^99m^Tc complexes with high stability both in aqueous solution and in plasma. Selective uptake and retention of ^99m^Tc-NS_3_M1 in tumors suggests that this agent is promising as a candidate for imaging tumor hypoxia; however, ^99m^Tc-NS_3_M2 had an unfavorable in vivo profile (1). This chapter summarizes the data obtained with ^99m^Tc-NS_3_M1.

### Related Resource Links:

Hypoxia imaging agents (http://www.ncbi.nlm.nih.gov/books/?term=hypoxia+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD

Hypoxia-related articles (http://www.ncbi.nlm.nih.gov/omim/?term=hypoxia) in Online Mendelian Inheritance in Man (OMIM)

Bioassy information on hypoxia (http://www.ncbi.nlm.nih.gov/pcassay?term=hypoxia) in PubChem

Hypoxia-related compounds (http://www.ncbi.nlm.nih.gov/pcsubstance?term=hypoxia) in PubChem

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22534030)]

Synthesis of the ligands M1 and M2 was achieved by reaction of the corresponding amino derivatives of metronidazole with succinimide derivative of 4-isocyanobutanoic acid (1). The chemical yields were 42% and 72% for M1 and M2, respectively. Labeling through formation of ^99m^Tc-(4+1) complexes was performed by substitution with ^99m^Tc-EDTA/mannitol as precursor (radiochemical purity >90%) and with M1 or M2 and tetradentate tripodal NS_3_ as coligands for 30 min at 70ºC. High-performance liquid chromatography (HPLC) analysis of the labeling mixture revealed the formation of a main product, with a retention time of 14.3 min and 17.5 min for ^99m^Tc-NS_3_M1 and ^99m^Tc-NS_3_M2, respectively. The radiochemical purity was >90% for both agents. The structure of ^99m^Tc complexes was corroborated using stable rhenium as a surrogate for technetium. The radiochemical yield and specific radioactivity were not reported. The partition coefficients (log P) between 1-octanol and phosphate buffer (pH 7.4) were 0.7 ± 0.1 and 1.2 ± 0.3 for ^99m^Tc-NS_3_M1 and ^99m^Tc-NS_3_M2, respectively.

^99m^Tc-NS_3_M1 and ^99m^Tc-NS_3_M2 were stable for >6 h in labeling milieu at room temperature. After incubation in human plasma for 4 h at 37°C, ^99m^Tc-NS_3_M1 and ^99m^Tc-NS_3_M2 were 95 ± 4% and 85 ± 2% intact, respectively.

Binding to plasma protein was studied with size-exclusion chromatography. ^99m^Tc-NS_3_M1 had relatively low protein binding (12 ± 1%), correlating with the high in vitro stability and low lipophilicity of this complex. However, the protein binding of ^99m^Tc-NS_3_M2 was extremely high (69 ± 3%), which might be partially explained by its higher lipophilicity.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22534030)]

In vitro uptake of ^99m^Tc-NS_3_M1 and ^99m^Tc-NS_3_M2 was evaluated under both normoxic and hypoxic conditions with cultured human colon adenocarcinoma HCT-15 cells (1). Cells were incubated at 37°C under an atmosphere of 95% air plus 5% carbon dioxide (aerobic exposure) or 95% nitrogen plus 5% carbon dioxide (hypoxic condition). After a 60-min equilibration period, the agents were added and incubated with the cells for another 60 min. A propidium iodide viability test showed that HCT-15 cells maintained >90% of viability for >90 min under hypoxic conditions. Both agents showed preferential uptake in hypoxia, with hypoxia/normoxia uptake ratios of 1.5 ± 0.2 and 1.4 ± 0.3 for ^99m^Tc-NS_3_M1 and ^99m^Tc-NS_3_M2, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22534030)]

Giglio et al. first evaluated the biodistribution of the two agents in normal CD1 mice (1). Animals were euthanized at 2 h and 4 h, respectively, after injection of 0.037–0.37 MBq (0.001–0.01 mCi) ^99m^Tc-NS_3_M1 or ^99m^Tc-NS_3_M2 (n = 3 mice/time point per agent). ^99m^Tc-NS_3_M1 showed low blood, lung, and liver uptake and was excreted through both the urinary and hepatobiliary tracts, as expected for a compound with intermediate lipophilicity. Thyroid and stomach radioactivities were very low, indicating minimal in vivo reoxidation of reduced Tc. Uptake in other organs was negligible. In contrast, ^99m^Tc-NS_3_M2 exhibited a very high liver activity, probably due to the high protein binding capability. Excretion was very low within the studied period. These results suggest that ^99m^Tc-NS_3_M2 has an unfavorable in vivo profile in normal animals. The detailed biodistribution data are presented in Table 2 of Giglio et al. (1).

Giglio et al. then evaluated the tumor uptake of ^99m^Tc-NS_3_M1 in C57BL/6 mice bearing 3LL Lewis murine lung carcinomas, but did not evaluate ^99m^Tc-NS_3_M2 because of its poor pharmacokinetics (1). Mice were euthanized at different time points (n = 3 mice/time point) after injection of 0.037–0.37 MBq (0.001–0.01 mCi). This animal model was selected because of the high degree of hypoxia within this tumor. ^99m^Tc-NS_3_M1 showed relatively high initial tumor uptake (2.5 ± 0.3% of injected dose per gram of tissue (ID/g) at 0.5 h after injection) and significant retention until 4 h (1.2 ± 0.2% ID/g at 4 h after injection). The tumor/muscle ratios were 2.8, 2.4, 2.4, and 2.0 at 0.5, 1, 2, and 4 h after injection, respectively. The tumor/blood ratios were 0.6, 0.6, 1.0, and 1.0 at 0.5, 1, 2, and 4 h after injection, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22534030)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22534030)]

No references are currently available.

## References

1 Giglio, J., et al., Synthesis, in vitro and in vivo characterization of novel (99m)Tc-'4+1'-labeled 5-nitroimidazole derivatives as potential agents for imaging hypoxia. Nucl Med Biol, 2012 April 23. [Epub ahead of print].
2 Chitneni S.K., et al. (2011). Molecular imaging of hypoxia. J Nucl Med.
3 Bollineni, V.R., et al., Hypoxia imaging using Positron Emission Tomography in non-small cell lung cancer: Implications for radiotherapy. Cancer Treat Rev, 2012
4 Kizaka-Kondoh S., Kuchimaru T., Kadonosono T. (2011). Pathophysiological response to hypoxia - from the molecular mechanisms of malady to drug discovery:hypoxia-inducible factor-1 (HIF-1)-active cells as a target for cancer therapy. J Pharmacol Sci.
5 Arabi M., Piert M. (2010). Hypoxia PET/CT imaging: implications for radiation oncology. Q J Nucl Med Mol Imaging.
6 Evans C.E., et al. (2011). Techniques of assessing hypoxia at the bench and bedside. Angiogenesis.
7 Sun X., et al. (2011). Tumor hypoxia imaging. Mol Imaging Biol.
8 Sharma R. (2011). Nitroimidazole radiopharmaceuticals in bioimaging: part I: synthesis and imaging applications. Curr Radiopharm.